# [NIe^4^,Asp^5^,D-Phe^7^, ^67^Ga/^68^Ga-1,4,7,10-tetraazacyclododecane-N,N’,N’’,N’’’-1,4,7,10-tetraacetic acid-Lys^11^]-α-MSH_4-11_

Chemical name: | [NIe^4^,Asp^5^,D-Phe^7^, ^67^Ga/^68^Ga-1,4,7,10-tetraazacyclododecane-N,N”,N”,N’’’-1,4,7,10-tetraacetic acid-Lys^11^]-α-MSH_4-11_
Abbreviated name: | ^67^Ga/^68^Ga-DOTA-NAPamide
Synonym: | ^67^Ga/^68^Ga-Labeled α-melanocyte−stimulating hormone analog, ^67^Ga/^68^Ga-NAPamide, [NIe^4^,Asp^5^,D-Phe^7^, ^67^Ga/^68^Ga-DOTA-Lys^11^]-α-MSH_4-11_
Agent Category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor, MC1R
Target Category: | Peptide-receptor binding
Method of detection: | Positron emission tomography (PET), planar gamma imaging, single-photon emission computed tomography (SPECT)
Source of signal: | ^67^Ga, ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Structure of ^67^Ga/^68^Ga-DOTA-NAPamide, the Lys-NH is a Lys-εNH. The Ga coordination configuration has not been confirmed by experiments.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gallium-labeled+alpha-melanocyte-stimulating+hormone+peptides)+OR+(radiolabeled-alpha-MSH))]

[NIe^4^,Asp^5^,D-Phe^7^, ^67^Ga/^68^Ga-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid- Lys^11^]-α-MSH_4-11_ (^67^Ga/^68^Ga-NAPamide) is a radioligand developed as a molecular imaging probe for primary and metastatic melanoma (1). ^67^Ga/^68^Ga-NAPamide is an α-melanocyte−stimulating hormone (MSH) peptide labeled with ^67^Ga or ^68^Ga. ^67^Ga is a gamma emitter with a physical half-life (t_½_) of 78.2 h and can be used for gamma imaging. ^68^Ga is a positron emitter with a physical t_½_ of 68 min and is suitable for positron emission tomography (PET).

Malignant melanoma is the sixth most common cancer in the United States (2). Early diagnosis and prompt surgical removal comprise the best approach for a possible cure (3). The melanocortin (MC) system is the best characterized neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (4). Most cutaneous cell types express MC receptors, proopiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Five MC receptors (MC-1 to MC-5) have been cloned and characterized as receptors that belong to the G-protein−coupled receptor superfamily. MSHs (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_) is a peptide of 13 amino acids and is the most potent, naturally occurring, melanotropic peptide (5). The biological effects of α-MSH are mediated via MC receptors.

Although PET imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (6, 7). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC-1 receptors that are overexpressed on human and mouse melanoma cells (6, 8-11). Some studies have successfully used 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) coupled to the α-MSH peptide analogs for radiolabeling. These α-MSH derivatives (DOTA-α-MSH) can be labeled with a variety of radionuclides (6). Froidevaux et al. (12) reported the synthesis of ^111^In-DOTA-[Nle^4^-D-Phe^7^]-α-MSH (^111^In-DOTA-NAP-MSH) and ^111^In-[βAla^3^,Nle^4^,Asp^5^,D-Phe^7^,Lys^10^]-α-MSH_3-10_ (^111^In-DOTA-MSH_OCT_) that exhibited high affinity for the MC-1 receptors in mice bearing B16F1 melanomas. To improve the tumor/kidney uptake ratio, the same group of researchers designed a short linear α-MSH analog, NAPamide, with a net charge of +1 and DOTA conjugated to the C-terminal lysine (1). They radiolabeled DOTA-NAPamide with either ^67^Ga or ^68^Ga as a potential molecular imaging probe to target melanoma.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Gallium-labeled+alpha-melanocyte-stimulating+hormone+peptides)+OR+(radiolabeled-alpha-MSH)+)+AND+synthesis)]

Froidevaux et al. (1) reported the synthesis of ^67^Ga/^68^Ga-NAPamide.The NAPamide peptide analog was synthesized by continuous-flow technology and the standard 9-fluorenylmethoxycarbonyl (Fmoc)/O-benzotriazolyl-tetramethyluronium hexafluorophosphate chemistry on rink amide 4-methylbenzhydrylamine resin (13, 14). The purity of NAPamide was >95%. NAPamide was then conjugated to DOTA by adding the peptide in N,N’-diisopropylethylamine/diemthylformamide (DMF) to DOTA that was preincubated for 10 min with O-[7-azabenzotriazole-1-yl]-1,1,3,3-tetramethyluronium hexafluorophosphate/DMF. The mixture was incubated for 1 h at room temperature. The peptide conjugate was then precipitated in ice-cold diethyl ether. DOTA was deprotected by mixing this peptide conjugate with trifluoroacetic acid, thioanisole, water, and 1,2-ethanedithiol. The reaction mixture was stirred for 4 h, and the deprotected DOTA-NAPamide was precipitated with ice-cold diethyl ether. This was purified by high-performance liquid chromatography (HPLC) before radiolabeling. The purity of DOTA-NAPamide was >99% with a 15% overall yield. The molecular weight was confirmed as 1,485.5 (compared to the calculated value of 1,485.7) by mass spectrometry. For ^67^Ga labeling, ^67^Ga-chloride was added to the DOTA-NAPamide in acetate buffer containing gentisic acid. The mixture was incubated for 30 min at 95ºC. After purification on a Sep-Pak C_18_ cartridge, the specific activity was >7.4 GBq/μmol (0.2 Ci/μmol). The yield and radiochemical purity were not reported. For ^68^Ga labeling, ^68^Ga in 0.5 N hydrochloric acid was obtained from the ^68^Ge/^68^Ga generator; 1 mmol Ga^3+^ was added, and the mixture was evaporated to dryness. After redissolving in acetate buffer (pH 4.8), DOTA-NAPamide was added. The mixture was heated for 15 min at 90ºC. After purification on a Sep-Pak C_18_ cartridge, the radiochemical purity was >98%. The yield and specific activity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Gallium-labeled+alpha-melanocyte-stimulating+hormone+peptides)+OR+(radiolabeled-alpha-MSH))+AND+in+vitro)]

Froidevaux et al. (1) conducted in vitro competitive receptor-binding studies (n = 3–9) of unlabeled NAPamide and DOTA-NAPamide with mouse B16F1 melanoma cells that express the MC-1 receptor. The inhibition concentrations (IC_50_) were determined to be 0.27 ± 0.07 nM and 1.37 ± 0.35 nM for NAPamide and DOTA-NAPamide, respectively. In comparison, the IC_50_ for DOTA-MSH_OCT_ (DOTA attached to the N-terminal end) was 9.21 ± 1.27 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Gallium-labeled+alpha-melanocyte-stimulating+hormone+peptides)+OR+(radiolabeled-alpha-MSH))+AND+rodentia)]

In vivo biodistribution studies of ^67^Ga-NAPamide were performed in B6D2F1 mice bearing a primary s.c. B16F1 murine melanoma (1). Each mouse received 185 kBq (5 μCi) ^67^Ga-NAPamide intravenously. The radioactivity levels in percent injected dose per gram (% ID/g) in the B16F1 tumor (n = 4–8) were 9.43 ± 1.06 (4 h), 3.10 ± 0.36 (24 h), and 1.61 ± 0.20 (48 h). The kidney radioactivity levels (% ID/g) were lower than the tumor levels: 3.98 ± 0.10 (4 h), 2.04 ± 0.17 (24 h), and 1.24 ± 0.09 (48 h). The radioactivity levels (% ID/g) in the liver were relatively low: 0.28 ± 0.02 (4 h), 0.25 ± 0.02 (24 h), and 0.23 ± 0.02 (48 h). At 4 h, the radioactivity levels (% ID/g) in other major organs were 0.26 ± 0.03 (blood), 0.05 ± 0.01 (muscle), 0.16 ± 0.02 (small intestine), 0.20 ± 0.03 (lung), 0.36 ± 0.05 (bone), and 0.19 ± 0.02 (skin). At 24 h, these levels (% ID/g) decreased to 0.06 ± 0.01 (blood), 0.02 ± 0.00 (muscle), 0.13 ± 0.02 (small intestine), 0.09 ± 0.01 (lung), 0.28 ± 0.03 (bone), and 0.11 ± 0.02 (skin). When 15 mg L-lysine was coinjected with ^67^Ga-NAPamide, the kidney radioactivity level was decreased by 64%, whereas the radioactivity levels in other major organs were not affected. Coinjection with 50 μg α-MSH reduced the 4-h tumor radioactivity level by >80%. In a separate study to evaluate the effect of the quantity of injected peptide on the pattern of distribution, mice bearing the B16F1 melanoma were injected with a mixture of varied quantities of nonradioactive Ga-DOTA-NAPamide (20, 170, or 420 pmol) with ^67^Ga-DOTA-NAPamide (1). At 4 h, the tumor radioactivity levels (n = 3–4) were reduced by 5-fold with injection of 420 pmol peptide compared to the peptide dose of 20 pmol. The radioactivity level in the kidney decreased by only 1.4-fold for the same peptide doses. No peptide dose effects were observed in other normal tissues.

Froidevaux et al. (1) conducted autoradiography of ^67^Ga-NAPamide in mice (n = 5) bearing the primary B16F1 tumor or metastatic lung/liver tumors induced by i,v, injection of B16F1 cells. Each mouse was given a dose of 740 kBq (20 μCi) ^67^Ga-DOTA-NAPamide. The mice were euthanized 4 h after injection. Autoradiographs identified selective radioactivity accumulation of ^67^Ga-DOTA-NAPamide in the melanoma lesions identified in the lung, liver, and skin. The radioactivity level in the primary skin lesions was similar to the metastatic lung lesions. There was also a uniform distribution of the radioactivity throughout the tumor.

PET imaging of mice bearing the B16F1 melanoma in their right flank was conducted with i.v. injection of 40 pmol (50.1 GBq/μmol or 1.35 Ci/μmol) ^68^Ga-NAPamide (1). There was a rapid tumor radioactivity uptake and fast blood clearance via the kidneys. At 0.5 h, only the tumor, kidney, bladder, and the heart were visible. Whereas the tumor radioactivity level remained unchanged up to 3 h, the radioactivity levels in the heart and kidney decreased. The optimum tumor/normal tissue contrast was at 1 h. Kidney and tumor radioactivity levels were also measured from tissue samples collected (n = 2–4) at 0.5, 1, 2, and 3 h. The tumor radioactivity level of ^68^Ga-NAPamide remained constant at ~7% ID/g between 0.5–3 h. The kidney radioactivity level dropped by 35% from ~4.6% ID/g at 0.5 h to ~3% at 1 h (extrapolated from Figure 5C in Froidevaux et al. (1)). At the higher peptide dose of 290 pmol (16.5 GBq/μmol or 0.45 Ci/μmol), ^68^Ga-NAPamide deceased the tumor radioactivity level to ~2.5% ID/g at 0.5–3 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Gallium-labeled+alpha-melanocyte-stimulating+hormone+peptides)+OR+(radiolabeled-alpha-MSH))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Gallium-labeled+alpha-melanocyte-stimulating+hormone+peptides)+OR+(radiolabeled-alpha-MSH))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Gallium-labeled+alph(a-melanocyte-stimulating+hormone+peptides)+OR+(radiolabeled-alpha-MSH))+AND+human)]

No publication is currently available.

## References

1 Froidevaux S., Calame-Christe M., Schuhmacher J., Tanner H., Saffrich R., Henze M., Eberle A.N. (2004). A gallium-labeled DOTA-alpha-melanocyte- stimulating hormone analog for PET imaging of melanoma metastases. J Nucl Med.
2 Miao Y., Benwell K., Quinn T.P. (2007). 99mTc- and 111In-labeled alpha-melanocyte-stimulating hormone peptides as imaging probes for primary and pulmonary metastatic melanoma detection. J Nucl Med.
3 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
4 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
5 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
6 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
7 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
8 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
9 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
10 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
11 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
12 Froidevaux S., Calame-Christe M., Tanner H., Sumanovski L., Eberle A.N. (2002). A novel DOTA-alpha-melanocyte-stimulating hormone analog for metastatic melanoma diagnosis. J Nucl Med.
13 Froidevaux S., Calame-Christe M., Tanner H., Eberle A.N. (2005). Melanoma targeting with DOTA-alpha-melanocyte-stimulating hormone analogs: structural parameters affecting tumor uptake and kidney uptake. J Nucl Med.
14 Cheng Z., Zhang L., Graves E., Xiong Z., Dandekar M., Chen X., Gambhir S.S. (2007). Small-Animal PET of Melanocortin 1 Receptor Expression Using a 18F-Labeled {alpha}-Melanocyte-Stimulating Hormone Analog. J Nucl Med.